# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Asp–Tyr(SO_3_H)–Met–Gly–Trp–Met–Asp–Phe–NH_2_

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Asp–Tyr(SO_3_H)–Met–Gly–Trp–Met–Asp–Phe–NH_2_
Abbreviated name: | ^111^In-DOTA-sCCK8
Synonym:
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gastrin+analogs)]

The gastrointestinal peptides gastrin and cholecystokinin-2 (CCK2) have various regulatory functions in the brain and gastrointestinal tract (1). Gastrin and CCK2 have the same COOH-terminal pentapeptide amide sequence GWMDF-NH_2_, which is the biologically active site (2). Human gastrin is a peptide composed of 33 amino acids and also exists in several C-terminal–truncated forms (3). These truncated forms include minigastrin (MG0), which is a 13-residue peptide with the sequence of D–Glu–Glu–Glu–Glu–Glu–Glu–Ala–Tyr–Gly–Trp–Met–Asp–Phe–NH_2_. CCKs exist in a variety of biologically active molecular fragments ranging from 4 to 18 amino acids and including sulphated and unsulphated CCK8, which is an octapeptide (DYMGWMDF-NH_2_) (4). Two CCK receptor subtypes have been identified in normal tissues by their binding affinities to gastrin. CCK1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK2 (CCK-B, brain) receptors have high affinity for gastrin (4). The sulphated CCK8 peptide displays high affinity for both CCK1 and CCK2 receptors, which are G-protein–coupled (5). These receptors have also been found to be overexpressed in a variety of tumor types (5). CCK2 receptors have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (1). CCK1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas. Radiolabeled CCK8 peptides have been studied in tumors expressing CCK2 receptors with good specificity for potential in vivo imaging.

Hellmich et al. (6) discovered a splice variant version (CCK2i4svR) of the CCK-2 receptor, which is expressed constitutively in human colorectal and pancreatic cancer (7, 8). A sulfated pan-CCKR-binding peptide, Asp–Tyr(SO_3_H)–Met–Gly–Trp–Met–Asp–Phe–NH2 (sCCK8), was N-terminally conjugated with tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) for radiolabeling with ^111^InCl_3_ to form ^111^In-DOTA-sCCK8 for imaging CCK2R and CCK2i4svR expressing tumors (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+synthesis)]

The peptide sequence Asp–Tyr(SO_3_H)–Met–Gly–Trp–Met–Asp–Phe–NH_2_ was obtained from a commercial source (Sigma-Aldrich, St. Louis, MO). The N-terminus was conjugated with a DOTA chelating group to produce DOTA-sCCK8 by N-hydroxysuccinimidyl-DOTA) (9). DOTA-sCCK8 was purified by reverse-phase high-performance liquid chromatography. Radiolabeling was performed by mixing ^111^InCl_3_ in ammonium acetate with DOTA-sCCK8. The mixture was heated at 80ºC for 30 min. The radiochemical purity and specific activity were 98% and 12 TBq/mmol (324 Ci/mmol), respectively. The labeling yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+in+vitro)]

An in vitro receptor-binding assay of ^111^In-DOTA-sCCK8 was performed on HEK293 cells transfected with the CCK-2R (HEK293-CCK2R) and CCK2i4svR (HEK293-CCK2i4svR) (9). Binding of ^111^In-DOTA-sCCK8 to CCK2R and CCK2i4svR was 26.9 ± 2.1% and 29.7 ± 0.6% incubation dose (ID) after 60 min of incubation at room temperature, respectively. Incubation with an excess of sCCK8 resulted in 4.0 ± 3.1% ID and 2.3 ± 0.4% ID, respectively. For ^111^In-DOTA-MG0, binding was 31.5 ± 1.6% ID and 24.4 ± 0.1% ID (CCK2R and CCK2i4svR, respectively). Receptor binding in the presence of an excess sCCK8 binding was 3.1 ± 0.4 and 2.4 ± 1.0% ID, respectively. Binding to non-transfected control HEK293 cells was negligible for both peptides (<0.7% ID). The inhibition constant (K_i_) values of DOTA-sCCK8 were 14.2 nM for CCK2R and 1.8 nM for CCK2i4svR. In comparison, the K_i_ values of DOTA-MG0 were 128 nM for CCK2R and 10.4 nM for CCK2i4svR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+rodentia)]

Laverman et al. (9) performed biodistribution studies of ^111^In-DOTA-sCCK8 in nude mice bearing either a HEK293-CCK2R tumor or HEK293-CCK2i4svR tumor. Each mouse received 370 kBq (10 nCi) of ^111^In-DOTA-sCCK8 by i.v. injection. The tumor radioactivity levels at 2 h (n = 4) were 3.45 ± 0.69% injected dose per gram (ID/g) for HEK293-CCK2R and 2.91 ± 0.44% ID/g for HEK293-CCK2i4svR (P = 0.3). The uptake in both tumors were blocked by excess sCCK8 to <1.3% ID/g. Specific uptake (~90%) was also observed in the pancreas and stomach. The kidney radioactivity levels (3.21 ± 0.39% ID/g) were not blocked by sCCK8. The tumors have the highest uptake, followed by the pancreas, kidney and stomach. The blood and liver radioactivity levels were <0.5% ID/g. In comparison, the tumor radioactivity level of ^111^In-DOTA-MG0 at 2 h was 6.09 ± 0.65% ID/g for HEK293-CCK2i4svR tumor and was significantly higher than ^111^In-DOTA-sCCK8 (P = 0.001). However, the tumor accumulation was similar for both tracers (3.21% ID/g and 3.01% ID/g for ^111^In-DOTA-sCCK8 and ^111^In-DOTA-MG0, respectively) at 24 h. On the other hand, kidney accumulation of ^111^In-DOTA-MG0 was >17-fold and 11-fold higher than ^111^In-DOTA-sCCK8 at 2 and 24 h, respectively. Except for ^111^In-DOTA-sCCK8 at 2 h, kidney accumulation for both tracers was significantly reduced by ~30% in the presence of an excess unlabelled peptide at both 2 h and 24 h after injection. No pancreas uptake was observed for the ^111^In-DOTA-MG0, most likely because of its CCK2R selectivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sCCK8+and+human)]

No publication is currently available.

## References

1 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
2 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
3 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Hellmich M.R., Rui X.L., Hellmich H.L., Fleming R.Y., Evers B.M., Townsend C.M. (2000). Human colorectal cancers express a constitutively active cholecystokinin-B/gastrin receptor that stimulates cell growth. J Biol Chem.
7 Smith J.P., Stock E.A., Wotring M.G., McLaughlin P.J., Zagon I.S. (1996). Characterization of the CCK-B/gastrin-like receptor in human colon cancer. Am J Physiol.
8 Smith J.P., Verderame M.F., McLaughlin P., Martenis M., Ballard E., Zagon I.S. (2002). Characterization of the CCK-C (cancer) receptor in human pancreatic cancer. Int J Mol Med.
9 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.